# Anti-human sperm protein 17 monoclonal antibody-indocyanine green derivative 02

Chemical name: | Anti-human sperm protein 17 monoclonal antibody-indocyanine green derivative 02
Abbreviated name: | Anti-Sp17-ICG-Der-02
Synonym: | ICG-Der-02-Anti-Sp17
Agent category: | Antibody
Target: | Sperm protein 17 (Sp17 or Spa17)
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Indocyanine green derivative 02 (ICG-Der-02)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAK20878.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/221316733) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/53340) for more information about Sp17.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive complement to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (5-8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

Sperm protein 17 (Sp17) is expressed exclusively in the testes, with its primary function of binding to the zona pellucida for fertilization (9). Expression of Sp17 in other normal tissues is limited. However, Sp17 was later found to be aberrantly expressed in various malignant tumors, such as myeloma, ovarian tumors, and esophageal squamous cell tumors (10, 11). Sp17 was expressed in 66% of endometrial tumors and 61% of cervical tumors (12). Li et al. (13) explored the overexpression of Sp17 in malignant tumors as a molecular biomarker for tumor imaging by coupling anti-human Sp17 monoclonal antibody with ICG derivative 02 (anti-Sp17-ICG-Der-02). ICG-Der-02 contains one carboxyl functional group for covalent conjugation to the amino group of biomolecules. ICG-Der-02 exhibits favorable water solubility and higher fluorescence quantum yield than ICG. Anti-Sp17-ICG-Der-02 was evaluated for in vivo NIR imaging of Sp17-positive human hepatocellular carcinoma cell line SMMC-7721 xenografts in mice.

### Related Resource Links:

- Chapters in MICAD (ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), Sp17 (http://www.ncbi.nlm.nih.gov/books?term=Sp17%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Sp17 (http://www.ncbi.nlm.nih.gov/gene/53340))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Sp17 (http://www.ncbi.nlm.nih.gov/omim/608621))
- Clinical trials (ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02)]

Anti-Sp17 (clone 3C12, 1.3 nmol) was incubated with ICG-Der-02-N-hydroxysuccinimide ester (15 nmol) for 10 h at 4°C (13). Anti-Sp17-ICG-Der-02 was purified with dialysis. The absorption and emission peaks of anti-Sp17-ICG-Der-02 were at 780 nm and 835 nm, respectively. The absorption and emission peaks of ICG-Der-02 were at 780 nm and 810 nm, respectively. The immunoreactivity of anti-Sp17-ICG-Der-02 was ~60% compared with the unconjugated antibody. The number of ICG-Der-02 molecules per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02%20and%20in%20vitro)]

Immunocytochemical analysis showed that anti-Sp17 mainly localized on the surface of cultured SMMC-7721 cells (Sp17-positive) but not on the surface of cells from the human ovarian cancer cell line HO8910 (Sp17-negative) (13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02%20and%20rodentia)]

Tumor-imaging studies of anti-Sp17-ICG-Der-02 were performed in nude mice (n = 5) bearing SMMC-7721 tumors (13). Whole-body fluorescence images were obtained at 1 h and at 1, 2, 3, 5, and 7 d after intravenous injection of anti-Sp17-ICG-Der-02 (~6 nmol ICG-Der-02/mouse). Maximum NIR fluorescence signals in the tumors were obtained at 1 d after injection. Strong signal in the tumors was still observed at 7 d. On the other hand, ICG-Der-02 (n = 3) showed weak accumulation of NIR fluorescence signal in the tumors at 1 d and 2 d after injection. Both agents showed strong signals in the liver, kidney, and urinary bladder. Immunohistochemical analysis of the tumor sections showed that anti-Sp17 mainly localized on the cell surface and in the cytoplasm of the tumor tissues. No blocking studies with unconjugated anti-Sp17 were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sp17%20ICG-Der-02%20and%20human)]

No publication is currently available.

## Human Studies

Intramural Research Program

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
6 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
7 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
8 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
9 Wen Y., Richardson R.T., Widgren E.E., O'Rand M.G. (2001). Characterization of Sp17: a ubiquitous three domain protein that binds heparin. Biochem J.
10 De Jong A., Buchli R., Robbins D. (2002). Characterization of sperm protein 17 in human somatic and neoplastic tissue. Cancer Lett.
11 Li F.Q., Han Y.L., Liu Q., Wu B., Huang W.B., Zeng S.Y. (2009). Overexpression of human sperm protein 17 increases migration and decreases the chemosensitivity of human epithelial ovarian cancer cells. BMC Cancer.
12 Li F.Q., Liu Q., Han Y.L., Wu B., Yin H.L. (2010). Sperm protein 17 is highly expressed in endometrial and cervical cancers. BMC Cancer.
13 Li F.Q., Zhang S.X., An L.X., Gu Y.Q. (2011). In vivo molecular targeting effects of anti-Sp17- ICG-Der-02 on hepatocellular carcinoma evaluated by an optical imaging system. J Exp Clin Cancer Res.